# Avidin conjugated to tetramethyl-6-carboxyrhodamine-QSY^®^7

Chemical name: | Avidin conjugated to tetramethyl-6-carboxyrhodamine-QSY^®^7
Abbreviated name: | Av-TM-Q7
Synonym:
Agent Category: | Receptor ligand
Target: | D-galactose receptor
Target Category: | Receptor
Method of detection: | Optical imaging: fluorescence
Source of signal / contrast: | Tetramethyl-6-carboxyrhodamine
Activation: | Yes
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=Nucleotide&dopt=GenBank&val=13397825) sequence of Gallus gallus (chicken) avidin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorophore+quencher+optical+probes)]

Early detection of cancer helps in the development of a proper treatment and monitoring regimen that may result in a suitable prognosis for the patient (1-3). Although invasive methods are often used for the detection of cancer, they have limitations because these procedures may detect the neoplasm only in a specific location and cannot determine whether the cancer has metastasized to other parts of the body. Also, the various imaging techniques and modalities available for the non-invasive detection of cancer have low sensitivity and/or resolution that are insufficient to detect and quantify microscopic tumors or a small cluster of cancerous cells (4). In addition, some of the contrast agents used for imaging purposes are known to have toxic side effects (5). An attractive alternative to radionuclides or contrast agents is the use of fluorescent optical imaging agents that can be used to visualize and manage or treat clinical pathology, including that of cancer (6-9). However, fluorescent dyes used for imaging can be toxic or nonspecific, and the signal generated by these agents may be masked by autofluorescence, leading to a low signal/background ratio (10). Also, the attenuation of the fluorescent signal in the tissue is such that only superficial tumors can be detected in humans. Investigators have proposed the use of targeted fluorescent probes as a solution to improve the signal/background ratio with the optical imaging agents, and they have shown that fluorescence dye conjugated to avidin can be used to detect submillimeter disseminated peritoneal tumors under in vitro and in vivo conditions only if direct access to the peritoneal tumor is possible (11, 12). In addition to binding to biotin, avidin (a 68-kD tetrameric glycoprotein) is also known to bind to the D-galactose receptor, which belongs to the lectin class of molecules (proteins that can bind to the carbohydrate groups of glycoproteins and glycolipids) and has been reported to be expressed on the surface of ovarian, gastric, colon, and pancreatic cancer tumor cells (12, 13). Because of its specificity to bind to cell-surface ligands, the use of avidin-therapeutic drug conjugates as a method to deliver and facilitate the uptake of anticancer drugs by cancer cells was also suggested to treat this ailment (14). The net positive charge on avidin facilitates its binding to lectins or similar molecules that are negatively charged at physiological pH (11). Lectin-bound avidin or its conjugates are rapidly internalized by the cell, and the unbound avidin and its conjugates are quickly cleared from circulation through the liver. Therefore, this phenomenon helps generate very high target signal/background ratios in small animals (11).

Ogawa et al. proposed the use of fluorophores that could be activated only after binding to the target to further improve the target/background ratios obtained with the optical imaging agents (15). These investigators developed a targeted and activatable fluorophore-quencher (FQ) probe that could be used for the optical imaging of tumors. In the native state the signal from the fluorophore is quenched by a quencher molecule. A fluorescence signal would be obtained from the fluorophore only after the FQ probe was bound to, internalized, and activated by the target cells. The mechanism of quenching and generating fluorescence from the FQ probe is discussed elsewhere (16). Ogawa et al. investigated the use of tetramethyl-6-carboxyrhodamine (TAMRA, fluorophore)-QSY^®^7 (quencher) pair conjugated to avidin (Av-TM-Q7) for the detection of cancer cells under in vitro conditions and also in mice bearing SHIN3 cell line (of human ovarian cancer origin; these cells have a surface expression of the D-galactose receptor) tumors (15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TAMRA+QSY7+avidin+synthesis)]

The synthesis of Av-TM-Q7 was described by Ogawa et al. (15). Briefly, avidin was incubated with TAMRA-hydroxysuccinimide (NHS) ester in 0.1 M sodium phosphate buffer (Na_2_HPO_4_) (pH 8.5) for 30 min at room temperature. The Av-TM conjugate was purified on a Sephadex G50 column. The purified product was concentrated and added to a solution of QSY^®^7-NHS in dimethylsulfoxide. The mixture was incubated as described above. The final product, Av-TM-Q7, was purified on a Sephadex G25 column and stored at 4°C until required. The stability of Av-TM-Q7 under these storage conditions was not reported. Approximately three and five molecules of TAMRA and QSY^®^7, respectively, were reported to be conjugated to each molecule of avidin, as determined with a UV-visible spectroscopy system.

To generate a control conjugate for use in some studies, Av-TM-Q7 was incubated with disuccinimidyl suberate (DSS) in 0.1 M Na_2_HPO_4_ buffer (pH 8.5) for 1 h at room temperature. Incubation with the DSS generated a cross-linked avidin tetramer (Av-TM-Q7 (CL)) that does not degrade in the lysosome under acidic conditions. The purification and stability of Av-TM-Q7 (CL) was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Avidin+TAMRA+QSY7+in+vitro)]

The quenching ability of Av-TM-Q7 was determined by exposing the conjugate to 5% sodium dodecylsulfate (SDS), which is known to dissociate the avidin tetramer into its component monomers, in phosphate-buffered saline at room temperature for 10 min (15). For comparison, the Av-TM-Q7 (CL) conjugate was also treated with SDS under the same conditions. Measurement of the fluorescence signal from each native and denatured sample showed that only the dissociated sample of Av-TM-Q7 had a 40-fold increase in the signal intensity over background. Little change was noted in the signal obtained from Av-TM-Q7 (CL) with or without the SDS treatment.

To demonstrate activation of Av-TM-Q7 or the Av-TM-Q7 (CL) conjugates, SHIN3 cells were exposed to the respective conjugates at 37°C for 6 h to allow internalization and activation of the fluorophore in the lysosomes (15). Examination of the exposed cells under a fluorescence microscope showed that fluorescent dots were visible only in the lysosomes of cells exposed to Av-TM-Q7. No fluorescence signal was obtained from cells treated with the cross-linked conjugate. From these observations the investigators concluded that degradation of avidin in the lysosomes was responsible for generation of the fluorescent signal due to release of the quencher from the fluorophore in the Av-TM-Q7 conjugate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Avidin+TAMRA+QSY7+rodentia)]

Peritoneal tumors were generated in nude mice by intraperitoneal injections (i.p.) of either SHIN3 cells or SHIN3 cells transfected with a plasmid (ZsGreen) that constitutively expressed the green fluorescent protein (SHIN3/ZsGreen cells), and the tumors were allowed to grow for 3 weeks (15). Imaging was performed on the animals 3 h after an i.p. injection of the respective avidin conjugates. The number of animals injected per conjugate was not reported. Peritoneal tumors, including the submillimeter nodules, were visible only in mice treated with the Av-TM-Q7 conjugate. A considerably lower fluorescence signal was observed from tumors in mice treated with Av-TM-Q7 (CL).

To determine specificity of the Av-TM-Q7 and Av-TM-Q7 (CL) conjugates, mice with the SHIN3/ZsGreen cell tumors (the number of animals injected with each conjugate was not reported) were given an i.p. injection of either Av-TM-Q7 or Av-TM-Q7 (CL) (15). An almost complete overlap of the fluorescent signal from TAMRA and ZsGreen was reported in tumors of these animals. With results obtained from this study, it was concluded that Av-TM-Q7 could be used to visualize D-galactose receptor–positive tumors in the peritoneal cavity of mice.

On the basis of the information obtained from the various studies performed with Av-TM-Q7, the investigators concluded that this activatable fluorescence-quencher probe could be a promising agent to manage cancer with a “see and treat” strategy if an optical probe could be introduced into the peritoneum (15).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Avidin+TAMRA+QSY7+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Avidin+TAMRA+QSY7+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by the Intramural Research Program of the National Institutes of Health, National Cancer Institute, and the Center for Cancer Research.

## References

1 Brepoels L., Stroobants S. (2008). PET scanning and prognosis in Hodgkin's lymphoma. Curr Opin Oncol.
2 Dobbe E., Gurney K., Kiekow S., Lafferty J.S., Kolesar J.M. (2008). Gene-expression assays: new tools to individualize treatment of early-stage breast cancer. Am J Health Syst Pharm.
3 Kolesar J.M. (2008). Assessing therapeutically developed assays. Manag Care.
4 Frangioni J.V. (2008). New technologies for human cancer imaging. J Clin Oncol.
5 ten Dam M.A., Wetzels J.F. (2008). Toxicity of contrast media: an update. Neth J Med.
6 Xiao W., Yao N., Peng L., Liu R., Lam K.S. (2009). Near-infrared optical imaging in glioblastoma xenograft with ligand-targeting alpha 3 integrin. Eur J Nucl Med Mol Imaging.
7 Sampath L., Wang W., Sevick-Muraca E.M. (2008). Near infrared fluorescent optical imaging for nodal staging. J Biomed Opt.
8 van de Ven S.M., Elias S.G., van den Bosch M.A., Luijten P., Mali W.P. (2008). Optical imaging of the breast. Cancer Imaging.
9 Thekkek N., Richards-Kortum R. (2008). Optical imaging for cervical cancer detection: solutions for a continuing global problem. Nat Rev Cancer.
10 Aalders M.C. (1999). N. vd Vange, F.A. Stewart, M.G. Klein, M.J. vd Vijver, and H.J. Sterenborg, White-light toxicity, resulting from systemically administered 5-aminolevulinic acid, under normal operating conditions. J Photochem Photobiol B.
11 Hama Y., Urano Y., Koyama Y., Kamiya M., Bernardo M., Paik R.S., Krishna M.C., Choyke P.L., Kobayashi H. (2006). In vivo spectral fluorescence imaging of submillimeter peritoneal cancer implants using a lectin-targeted optical agent. Neoplasia.
12 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2006). Targeted optical imaging of cancer cells using lectin-binding BODIPY conjugated avidin. Biochem Biophys Res Commun.
13 Nakahara S., Raz A. (2008). Biological modulation by lectins and their ligands in tumor progression and metastasis. Anticancer Agents Med Chem.
14 Yao Z., Zhang M., Sakahara H., Saga T., Arano Y., Konishi J. (1998). Avidin targeting of intraperitoneal tumor xenografts. J Natl Cancer Inst.
15 Ogawa, M., N. Kosaka, M.R. Longmire, Y. Urano, P.L. Choyke, and H. Kobayashi, Fluorophore-Quencher Based Activatable Targeted Optical Probes for Detecting in Vivo Cancer Metastases. Mol Pharm, 2009
16 Lee S., Park K., Kim K., Choi K., Kwon I.C. (2008). Activatable imaging probes with amplified fluorescent signals. Chem Commun (Camb).